# 2-Hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7,-hexahydro-11bH-bezo[α]-quinolizine

Chemical name: | 2-Hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7,-hexahydro-11bH-bezo[α]-quinolizine
Abbreviated name: | [^11^C]DTBZ
Synonym: | [^11^C]Dihydrotetrabenazine
Agent category: | Compound
Target: | Type 2 vesicular monoamine transporter (VMAT2)
Target category: | Transporter
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29)]

Vesicular monoamine transporter (VMAT2) is present in brain monoaminergic neurons and is responsible for collecting neurotransmitters (dopamine, norepinephrine and serotonin) from the cytoplasm and storing them in vesicles for synaptic release (1). VMAT2 is therefore an essential regulator of monoaminergic neuronal function. In the brain, VMAT2 is highly present in the striatum, hypothalamus, substantia nigra, and hippocampus, with low levels in cerebellum and occipital cortex (2). In the striatum, greater 95% of VMAT2 is associated with dopaminergic neurons (3). Decreases in the VMAT2 level are implicated in movement disorders, such as Parkinson’s disease (PD), Alzheimer’s disease (AD) and Huntington disease (HD).

VMAT2 is highly expressed by β cells of the endocrine pancreas and not in exocrine pancreas. VMAT2 is expressed mainly on the β-cells in the islets of Langerhans and composed of 1-2% of the pancreatic mass. β-cell mass (BCM) is a useful indicator of the function of the pancreas. In type I diabetes, β-cells are destroyed leading to a dramatic decrease in BCM. In type II diabetes, there is a slow and insidious decrease in BCM because of peripheral insulin resistance and increase demand for insulin. Decreases in BCM in the human and monkey pancreases correlate to the decreases in insulin level in the blood. VMAT2 is a potential target for non-invasive assessment of BCM and pancreatic function.

VMAT2 has been studied in vivo by positron emission tomography (PET) using [^11^C]dihydrotetrabenazine (2-hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7,-hexahydro-11bH-bezo[α]-quinolizine) ([^11^C]DTBZ) with selective VMAT2 binding activity in neurons of the brain and pancreas . Binding of DTBZ to the vesicular monoamine transporter is stereospecific (4). The (+)-enantiomer showed a high affinity in vitro binding (K_i_ = 0.97 ± 0.48 nM) for the VMAT2 in rat brain striatum, whereas the (-)-enantiomer was inactive (K_i_ = 2.2 ± 0.3 μM). [^11^C]DTBZ has been developed as a PET agent for the non-invasive study of VMAT2 in the human brain.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VMAT2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (VMAT2 (http://www.ncbi.nlm.nih.gov/gene/6571))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/193001)
- Clinical trials (VMAT2 (http://www.clinicaltrials.gov/ct2/results?term=VMAT2))
- Drug information in FDA (VMAT2 (http://google2.fda.gov/search?q=VMAT2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29%20and%20synthesis)]

In the report by Jewett et al. (5), [^11^C]dihydrotetrabenazine (2-hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7,- hexahydro-11bH-bezo[α]-quinolizine) ([^11^C]DTBZ) [^11^C]DTBZ was synthesized by alkylation of the 9-hydroxy precursor 2-hydroxy-3-isobutyl-9-hydroxy-10-methoxy-1,2,3,4,6,7,-hexahydro-11bH-bezo[α]-quinolizine) with [^11^C]methyl iodide. Purification with column chromatography provided a radiochemical yield of 12% based on [^11^C]CO_2_, radiochemical purity >95%, and specific activity of 59-74 GBq/μmol (1.6-2.0 Ci/μmol) in 30 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29%20and%20in%20vitro)]

Henry et al. (2) reported that saturation binding experiments of [^3^H]DTBZ in the synaptic vesicles from murine striatum estimated a K_d_ value of 2.3 to 2.7 nM, with a B_max_ value of 1.35 pmol/mg protein. In vitro binding studies of human postmortem brain with [^3^H]DTBZ showed high binding in the caudate (766 fmol/mg protein), nucleus accumbens (751 fmol/mg protein), putamen (742 fmol/mg protein), substantia nigra (465 fmol/mg protein), hypothalamus (245 fmol/mg protein) pallidum (115-128 fmol/mg protein) hippocampus (83 fmol/mg protein) and frontal cortex (57 fmol/mg protein).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29%20and%20rodentia)]

Kilbourn et al. (4) reported ex vivo regional distribution studies in the brain of normal mice showing accumulation of radioactivity in the striatum, hypothalamus, hippocampus and cerebellum at 15 min after injection of (+)[^11^C]DTBZ, [^11^C]DTBZ or (-)[^11^C]DTBZ. The highest brain accumulation and regional contrast was shown for the (+)-enantiomer, with a low and uniform uptake for the (-)-enantiomer. The racemic mixture showed intermediate accumulation. Pretreatment with 10 mg/kg (+)DTBZ 10 min before (+)[^11^C]DTBZ injection in mice significantly reduced accumulation in the striatum and hypothalamus. Frey et al. (6) performed metabolic studies in rats after injection of [^3^H]DTBZ. The fraction of unchanged [^3^H]DTBZ in blood liver and brain, as determined by thin-layer chromatography, was 86%, 93%, and 99% at 15 min after injection, respectively. Collantes et al. (7) estimated a binding potential (BP) value of 1.10 ± 0.16 (n = 10) in the striatum in rats (+)[^11^C]DTBZ PET imaging. In the rats treated with 6-OHDA, the striatal BP was reduced to 0.05.

Simpson et al. (8) performed ex vivo biodistribution studies in normal rats that demonstrated accumulation of radioactivity in the pancreas (5.43 ± 0.19% ID/g), liver (3.28 ± 0.41% ID/g), kidney (2.73 ± 0.06% ID/g), small intestine (1.63 ± 0.24% ID/g), stomach (1.38 ± 0.04% ID/g), heart (0.68 ± 0.05% ID/g), lung (0.51 ± 0.12% ID/g) and brain (0.44 ± 0.12% ID/g) at 30 min after injection of (+)[^11^C]DTBZ. (+)[^11^C]DTBZ PET dynamic imaging for 60 min in a rodent model of diabetes in rats (treated with streptozotocin (STZ) to induced BCM loss and diabetes). Imaging sessions were performed at 6 day after STZ treatment. Reduced radioactivity in the pancreata of STZ-treated rats (n = 5) was observed as compared to the pancreata of control rats (n = 5). Immunochemistry of pancreata of STZ-treated rats showed reduced islet areas and frequencies as compared to the pancreata of control rats. There was also loss of VMAT2 and proinsulin expression throughout the STZ-treated pancreata.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29%20and%20%28primate%20not%20human%29)]

Collantes et al. (7) performed (+)[^11^C]DTBZ PET imaging in two monkeys and estimated BP values of 1.06 and 1.31 in the basal ganglia. MTPT treatment of one monkey exhibited a 39.7% reduction in the (+)[^11^C]DTBZ accumulation. Murthy et al. (9) performed whole-body (+)[^11^C]DTBZ PET imaging in five baboons with most of the injected radioactivity localized to the liver and lung, followed by the intestines, brain, and kidneys. Effective doses to adult female and male were estimated to be 0.0061 and 0.0070 mSv/MBq, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28dihydrotetrabenazine%20or%20DTBZ%29%20and%20human)]

Koeppe et al. (10-12) performed various human PET studies using Logan graphical analysis, nonlinear least-squares analysis, equilibrium analysis and two-tissue compartment model to be satisfactorily accounted for the cerebral kinetics of (+)[^11^C]DTBZ. Distribution volume (DV), binding potential (BP) and transport constant (K_1_) can be estimated from the accumulation of radioactivity in various brain regions as measurements of the integrity of the presynaptic neurons. Chan et al. (13) showed that [^11^C]DTBZ PET studies in 10 normal volunteers to be reproducible using Logan analysis. Occipital cortex or cerebellum can be used as the reference region. The fraction of unchanged [^11^C]DTBZ in plasma was 80, 64, and 47% at 10, 30, and 60 min, respectively.

Frey et al. (6) compared [^11^C]DTBZ PET scans of 15 normal subjects (age, 22-70 years) with 7 PD patients (age, 57-79, receiving antiparkinsonian medication). There were reductions of putamen DV with increasing age, corresponding to losses of 0.77% per year in VMAT2 binding. PD patients had significant reduction in DV in the putamen (-61%) and in the caudate nucleus (-43%). Later studies revealed there are significant correlations of [^11^C]DTBZ binding reduction with PD severity of motor functions (14). Reduction of striatal VMAT2 binding was shown in patients with multiple system atrophy, but not in patients with essential tremor. Bohnen et al. (15) reported that there was a significant reduction of DV in the caudate (-33%) anterior putamen (-56%) and posterior putamen (-75%) in HD patients (n = 19) compared with normal controls (n = 64).

Gilman et al. (16) used PET with (+)[^11^C]DTBZ to examine striatal VMAT2 density in 20 dementia patients with Lewy bodies (DLB), 25 with AD, and 19 normal elderly controls. Six DLB patients developed Parkinsonism at least 1 year before dementia (DLB/PD) and 14 developed dementia before Parkinsonism or at about the same time (DLB/AD). Striatal BP was decreased by 62 to 77% in the DLB/PD group and 45 to 67% in the DLB/AD compared to AD and control. BP was lower in the DLB/PD group than the DLB/AD. No differences were found between AD and control groups. Both DLB groups had an anterior to posterior binding deficit gradient relative to controls (posterior putamen > anterior putamen > caudate nucleus). The DLB/AD group showed significant binding asymmetry only in posterior putamen. Therefore, PET with (+)[^11^C]DTBZ differentiates DLB from AD, and decreased binding in AD may indicate subclinical DLB pathology in addition to AD pathology.

Goland et al. (17) compared pancreatic [^11^C]DTBZ PET scans of 9 normal subjects with 6 patients with long-standing type 1 diabetes. The pancreatic mean BP_ND_ values (estimated by the 2-parameter multilinear reference tissue model) decreased in patients (1.86 ± 0.05) to 86% of control values (2.14 ± 0.08) (P = 0.01). The functional binding capacity was decreased in patients (44 ± 11) to 40% of control values (109 ± 9) (P = 0.001). Thence, the changes in functional binding capacity and BP_ND_ were less than the near-complete loss of stimulated insulin secretion and BCM observed in the diabetic patients (P = 0.001) comparing to normal controls. The high nonspecific binding in the exocrine pancreas may appear to overestimate BCM with pancreatic [^11^C]DTBZ PET scans.

## NIH Support

M01 RR00042, P01 NS15655, P50 AG08671, R01 MH47611, U42 RR016629-04, R01 DK63567-03, P30 DK063608-02, RO1 DK077493

## References

1 Schuldiner S. (1994). A molecular glimpse of vesicular monoamine transporters. J Neurochem.
2 Henry J.P., Scherman D. (1989). Radioligands of the vesicular monoamine transporter and their use as markers of monoamine storage vesicles. Biochem Pharmacol.
3 Vander Borght T.M., Sima A.A., Kilbourn M.R., Desmond T.J., Kuhl D.E., Frey K.A. (1995). [3H]methoxytetrabenazine: a high specific activity ligand for estimating monoaminergic neuronal integrity. Neuroscience.
4 Kilbourn M., Lee L., Vander Borght T., Jewett D., Frey K. (1995). Binding of alpha-dihydrotetrabenazine to the vesicular monoamine transporter is stereospecific. Eur J Pharmacol.
5 Jewett D.M., Kilbourn M.R., Lee L.C. (1997). A simple synthesis of [11C]dihydrotetrabenazine (DTBZ). Nucl Med Biol.
6 Frey K.A., Koeppe R.A., Kilbourn M.R., Vander Borght T.M., Albin R.L., Gilman S., Kuhl D.E. (1996). Presynaptic monoaminergic vesicles in Parkinson's disease and normal aging. Ann Neurol.
7 Collantes M., Penuelas I., Alvarez-Erviti L., Blesa J., Marti-Climent J.M., Quincoces G., Delgado M., Ecay M., Martinez A., Arbizu J., Rodriguez-Oroz M.C., Obeso J., Richter J.A. (2008). Rev Esp Med Nucl.
8 Simpson N.R., Souza F., Witkowski P., Maffei A., Raffo A., Herron A., Kilbourn M., Jurewicz A., Herold K., Liu E., Hardy M.A., Van Heertum R., Harris P.E. (2006). Visualizing pancreatic beta-cell mass with [11C]DTBZ. Nucl Med Biol.
9 Murthy R., Harris P., Simpson N., Van Heertum R., Leibel R., Mann J.J., Parsey R. (2008). Whole body [11C]-dihydrotetrabenazine imaging of baboons: biodistribution and human radiation dosimetry estimates. Eur J Nucl Med Mol Imaging.
10 Koeppe R.A., Frey K.A., Kuhl D.E., Kilbourn M.R. (1999). Assessment of extrastriatal vesicular monoamine transporter binding site density using stereoisomers of [11C]dihydrotetrabenazine. J Cereb Blood Flow Metab.
11 Koeppe R.A., Frey K.A., Kume A., Albin R., Kilbourn M.R., Kuhl D.E. (1997). Equilibrium versus compartmental analysis for assessment of the vesicular monoamine transporter using (+)-alpha-[11C]dihydrotetrabenazine (DTBZ) and positron emission tomography. J Cereb Blood Flow Metab.
12 Koeppe R.A., Frey K.A., Vander Borght T.M., Karlamangla A., Jewett D.M., Lee L.C., Kilbourn M.R., Kuhl D.E. (1996). Kinetic evaluation of [11C]dihydrotetrabenazine by dynamic PET: measurement of vesicular monoamine transporter. J Cereb Blood Flow Metab.
13 Chan G.L., Holden J.E., Stoessl A.J., Samii A., Doudet D.J., Dobko T., Morrison K.S., Adam M., Schulzer M., Calne D.B., Ruth T.J. (1999). Reproducibility studies with 11C-DTBZ, a monoamine vesicular transporter inhibitor in healthy human subjects. J Nucl Med.
14 Frey K.A., Koeppe R.A., Kilbourn M.R. (2001). Imaging the vesicular monoamine transporter. Adv Neurol.
15 Bohnen N.I., Koeppe R.A., Meyer P., Ficaro E., Wernette K., Kilbourn M.R., Kuhl D.E., Frey K.A., Albin R.L. (2000). Decreased striatal monoaminergic terminals in Huntington disease. Neurology.
16 Gilman S., Koeppe R.A., Little R., An H., Junck L., Giordani B., Persad C., Heumann M., Wernette K. (2004). Striatal monoamine terminals in Lewy body dementia and Alzheimer's disease. Ann Neurol.
17 Goland R., Freeby M., Parsey R., Saisho Y., Kumar D., Simpson N., Hirsch J., Prince M., Maffei A., Mann J.J., Butler P.C., Van Heertum R., Leibel R.L., Ichise M., Harris P.E. (2009). 11C-dihydrotetrabenazine PET of the pancreas in subjects with long-standing type 1 diabetes and in healthy controls. J Nucl Med.